# [^123^I]Iomazenil

Chemical name: | [^123^I]Iomazenil
Abbreviated name: | [^123^I]IMZ
Synonym:
Agent Category: | Compound
Target: | Central-type benzodiazepine receptors (on neurons)
Target Category: | Ligand binding
Method of detection: | SPECT
Source of signal: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Other non-primate mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodine-123-iomazenil%5BAll%20Fields%5D)]

[^123^I]Iomazenil ([^123^I]IMZ) is a ligand displaying high affinity for central-type benzodiazepine receptors, with high brain uptake and little nonspecific binding. It is a useful marker of neuronal viability. [^123^I]IMZ has been successfully used as a probe for single photon emission computed tomography (SPECT) in numerous clinical studies of diseases such Alzheimer’s [PubMed], epilepsy [PubMed], or cerebral ischemia [PubMed], for which alterations of benzodiazepine receptors have been reported (1, 2).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodine-123-iomazenil%5BAll%20Fields%5D%20AND%20synthesis%5BAll%20Fields%5D)]

[^123^I]IMZ is readily available commercially. Details on its synthesis, however, are scarcely reported in the research literature. A possible preparation method is given by Eersels et al. (3), who recommend using a nucleophilic exchange rather than an electrophilic route because of the conjugation of the carbonyl group in iomazenil.

The reported method involves flushing (with N_2_) and heating (at 121°C for 25 min) a reaction mixture kit consisting of 1 mg of bromo-mazenil, 0.2 mg of SnSO_4_, 4 mg of 2,5-dihydroxybenzoic acid, and 5 mg of citric acid together with ^123^I (37MBq; 1mCi). The labeling yield obtained is between 80% and 90%. Additional purification of the radiochemical can be done by high-performance liquid chromatography (HPLC) separation, dilution with an isotonic citrate buffer (pH 4), filtration, and sterilization. This additional procedure increases the purity of [^123^I]IMZ to more than 97%, with an overall yield of 70-80%.

A comparison of the destannylation approach to the original ^123^I for the bromo-substitution route can be found in the article by Zea-Ponce et al. (4).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodine-123-iomazenil%5BAll%20Fields%5D%20AND%20%22in%20vitro%22%5BAll%20Fields%5D)]

The biodistribution, metabolism, and excretion of [^123^I]IMZ have been studied in rats, rabbits, and humans. Studies showed that in all of the species, [^123^I]IMZ was rapidly metabolized, and more than 90% of the administrated radioactivity was excreted within the first 24 h. For rats and humans, the dominant metabolites were found to be the acid metabolite (R-COOH), the glucuronide of the acid (R-COOH-Glc), and the free iodide (I-). In rabbits, R-COOH, the oxidative metabolite (R'-CH2COOH), and I- were found. On the basis of these findings, Yoshimura et al. (5) suggested that possible metabolic pathways of [^123^I]IMZ were hydrolysis, oxidation, conjugation, and de-iodination. Experimental data also showed that the metabolites of [^123^I]IMZ did not cross the blood-brain barrier.

Several studies aimed at determining the binding potential (defined as the ratio the receptor density and the binding affinity) of [^123^I]IMZ, using kinetic and equilibrium methods, can be found in the literature (6, 7). Using 12 postmortem samples of human brain, Abi-Dargham et al. (8) found that the SPECT in vitro measurements derived from the rate constants were consistent with SPECT in vivo measurements (9, 10). Simulation studies performed by Onishi et al. (11) using SPECT and blood data from six healthy volunteers and five patients suggested that, in the normal brain, the scan time at which a single SPECT image best represented the relative receptor binding was 3.0-3.5 h after injection. This finding was supported by data from the volunteers taking part in the study.

Binding potential values can also be obtained by reference tissue methods, using either one or several tissue compartment models (6). Nevertheless, such methods have limitations, in particular with low receptor densities. They generally yield lower values than conventional kinetic modeling using an arterial input function.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodine-123-iomazenil%5BAll%20Fields%5D%20AND%20%22rodentia%22%5BMeSH%5D)]

Research using rat models showed that [^123^I]IMZ was a useful marker of neuronal viability. In a study by Kaji et al. (12), neuronal DNA was still intact in the ischemic regions where [^123^I]IMZ accumulation was preserved, and [^123^I]IMZ had the potential to significantly detect the region with DNA scission as a reduction in lesion/normal ratios. Kuge et al. (13) showed that in rats with the cerebral artery occluded intraluminally, [^123^I]IMZ uptake markedly decreased in the infarct regions at 4 and 24 h after the insult.

Using [^125^I]IMZ, Morimoto et al. (14) investigated regional changes in central-type benzodiazepine receptors in the cortical dysplasia model of epilepsy in rats. In this study, pregnant rats were irradiated at day 17 of gestation with 1.2 Gy to produce cortical dysplasia in their pups. In vitro autoradiography with [^125^I]IMZ performed at 8 weeks after birth showed that [^125^I]IMZ binding was significantly decreased in various cortical regions of the in utero irradiated rats, including the bilateral frontal cortex (down to 92-93% of control); cingulate cortex (91-92%); hippocampal areas CA1 (95%), CA2 (94-95%), and CA4 (95-96%); and caudate/putamen (90-94%).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22iomazenil%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%29)]

To determine whether benzodiazepine receptor or regional cerebral blood flow (rCBF) imaging was more sensitive in the detection of epileptic foci, Kurokawa et al. (15) examined simultaneously the benzodiazepine receptor and rCBF distribution changes in hippocampal kindled rabbits with in vivo double tracer autoradiography using [^125^I]IMZ and ^99m^Tc-labeled hexamethylpropylene amine oxime (^99m^Tc-HMPAO). Visual and quantitative analyses showed that benzodiazepine receptor imaging was much more sensitive in the detection of epileptic foci than rCBF imaging and, therefore, more useful in clinical epilepsy.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iomazenil%5BAll%20Fields%5D%20AND%20%28primate%20NOT%20human%29)]

SPECT imaging with [^123^I]IMZ was shown to be a valuable means of quantifying central neuroreceptor density and affinity in baboons. Studies by Laruelle et al. (16, 17), who measured arterial and brain regional activities in three baboons after a single bolus injection of the benzodiazepine antagonist [^123^I]IMZ, showed the feasibility of quantitative measurement of benzodiazepine receptors by kinetic analysis of SPECT data and the inadequacy of empirical methods of analysis, such as counts ratios, to evaluate differences in receptor density.

In a study by Sybirska et al. (18), SPECT imaging with [^123^I]IMZ was also used to measure benzodiazepine neuroreceptor occupancy of the agonist lorazepam administered at supratherapeutic doses in monkeys. In this study, the effects of doses of lorazepam (cumulative dose, 0.5 mg/kg) higher than the therapeutic doses (0.03 mg/kg, i.v.) were examined in a stepwise displacement paradigm. Results strongly suggested that single, therapeutically relevant doses of lorazepam occupy a relatively small percentage (i.e., <3%) of benzodiazepine receptors, and that benzodiazepine binding sites have a significant (i.e., >97%) receptor reserve.

Zoghbi et al. (19) performed pharmacokinetics studies of [^123^I]IMZ in two hypothermic and three normothermic anesthetized monkeys and compared the results to those obtained with five healthy human volunteers. Data showed that, after intravenous injection, [^123^I]IMZ rapidly diffused outside the vascular bed and was cleared from the arterial plasma tri-exponentially, and that it was metabolized mainly to a polar radiometabolite in the human, whereas an additional lipophilic radiometabolite was detected in the monkey. Organ analysis from a monkey given [^123^I]IMZ showed that the parent compound was actively taken up by peripheral organs. The polar radiometabolite accumulated mainly in the bile and the kidneys, whereas the non-polar radiometabolite accumulated in the urine and kidneys.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=iodine-123-iomazenil%5BAll%20Fields%5D%20AND%20human)]

Human studies have shown the potential of [^123^I]IMZ for evaluating the neuronal viability (or damage) after an ischemic stroke (12). One example is the study by Moriwaki et al. (20) performed on 15 patients with angiographically confirmed, unilateral, severe occlusive lesions (occlusion or >70% stenosis) in the carotid system. Dong et al. (21) compared [^123^I]IMZ SPECT images with the cerebral blood flow, cerebral metabolic rate of oxygen (CMRO_2_), and cerebral metabolic rate of glucose (CMRGlc) by positron emission tomography in the chronic stage of ischemic stroke. They also showed that [^123^I]IMZ could assess neuronal damage after an ischemic insult to the brain.

SPECT studies by Dey et al. (22) on human brains showed a strong uptake of [^123^I]IMZ in a distribution consistent with benzodiazepine receptor binding (22). In this study, serial total body scans were obtained in healthy volunteers after thyroid blockade. Abdominal imaging showed significant activity retention within the urinary and gastrointestinal tracts consistent with excretion via these routes. The absorbed dose to the urinary bladder was calculated to be 0.19 mGy/MBq; to the lower large intestine, 0.079 mGy/MBq; to the upper large intestine, 0.066 mGy/MBq; and to the thyroid, 0.063 mGy/MBq.

Verhoeff et al. (23) calculated the absorbed radiation doses of [^123^I]IMZ in various human organs using whole-body scans, blood samples, and urine from seven adult humans and applied the MIRD method. The urinary bladder wall (0.15 mGy/MBq), lower large intestinal wall (0.071 mGy/MBq), testes (0.044 mGy/MBq), and upper large intestinal wall (0.038 mGy/MBq) received the highest absorbed doses. The average effective dose equivalent of [^123^I]IMZ was estimated to be 0.033 mSv/MBq..

Ito et al. (24) developed a simple, autoradiographic method for the quantification of benzodiazepine by using one SPECT scan and calibrated the standard input function with one blood sampling.

## References

1 Reisine TD, Wastek GJ, Speth RC, Bird ED, Yamamura HI. (1979). Alterations in the benzodiazepine receptor of Huntington's diseased human brain. Brain Res.
2 Owen F, Poulter M, Waddington JL, Mashal RD, Crow TJ. (1983). [3H]R05-4864 and [3H]flunitrazepam binding in kainate-lesioned rat striatum and in temporal cortex of brains from patients with senile dementia of the Alzheimer type. Brain Res.
3 Eersels J, Travis M, Herscheid D. (2005). Manufacturing I-123-radiopharnaceuticals. Pitfalls and Solutions. J Label Compd Radiopharm.
4 Zea-Ponce Y, Baldwin RM, Zoghbi SS, Innis RB. (1994). Formation of 1-[123I]iodobutane in labeling [123I]iomazenil by iododestannylation: implications for the reaction mechanism. Appl Radiat Isot.
5 Yoshimura H, Yanai A, Matsumoto H, Ida K, Kurami M, Yonekura Y, Torizuka K. (1995). [.
6 Millet P, Graf C, Buck A, Walder B, Ibanez V. (2002). Evaluation of the reference tissue models for PET and SPECT benzodiazepine binding parameters. Neuroimage.
7 Bremner JD, Baldwin R, Horti A, Staib LH, Ng CK, Tan PZ, Zea-Ponce Y, Zoghbi S, Seibyl JP, Soufer R, Charney DS, Innis RB. (1999). Quantitation of benzodiazepine receptor binding with PET [11C]iomazenil and SPECT [123I]iomazenil: preliminary results of a direct comparison in healthy human subjects. Psychiatry Res.
8 Abi-Dargham A, Laruelle M, Seibyl J, Rattner Z, Baldwin RM, Zoghbi SS, Zea-Ponce Y, Bremner JD, Hyde TM, Charney DS, et al. (1994). SPECT measurement of benzodiazepine receptors in human brain with iodine-123-iomazenil: kinetic and equilibrium paradigms. J Nucl Med.
9 Millet P, Graf C, Buck A, Walder B, Westera G, Broggini C, Arigoni M, Slosman D, Bouras C, Ibanez V. (2000). Similarity and robustness of PET and SPECT binding parameters for benzodiazepine receptors. J Cereb Blood Flow Metab.
10 Ito H, Kawashima R, Koyama M, Goto R, Sato K, Ono S, Fukuda H. (1997). A method for the quantification of benzodiazepine receptors by using 123I-iomazenil and SPECT with one scan and one blood sampling. Ann Nucl Med.
11 Onishi Y, Yonekura Y, Tanaka F, Nishizawa S, Okazawa H, Ishizu K, Fujita T, Konishi J, Mukai T. (1996). Delayed image of iodine-123 iomazenil as a relative map of benzodiazepine receptor binding: the optimal scan time. Eur J Nucl Med.
12 Kaji T, Kuge Y, Yokota C, Tagaya M, Inoue H, Shiga T, Minematsu K, Tamaki N. (2004). Characterisation of [123I]iomazenil distribution in a rat model of focal cerebral ischaemia in relation to histopathological findings. Eur J Nucl Med Mol Imaging.
13 Kuge Y, Hikosaka K, Seki K, Ohkura K, Nishijima KC, Kaji T, Ueno S, Tsukamoto E, Tamaki N. (2003). Characteristic brain distribution of 1-(14)C-octanoate in a rat model of focal cerebral ischemia in comparison with those of (123)I-IMP and (123)I-iomazenil. J Nucl Med.
14 Morimoto K, Watanabe T, Ninomiya T, Hirao T, Tanaka A, Onishi T, Tamagami H. (2004). Quantitative evaluation of central-type benzodiazepine receptors with [(125)I]Iomazenil in experimental epileptogenesis: II. The rat cortical dysplasia model. Epilepsy Res.
15 Kurokawa K, Jibiki I, Matsuda H, Fukushima T, Tsuji S, Yamaguchi N, Hisada K. (1994). Comparison of benzodiazepine receptor and regional cerebral blood flow imaging of epileptiform foci in hippocampal kindled rabbits: a study with in vivo double tracer autoradiography using 125I-iomazenil and 99mTc-HMPAO. Brain Res.
16 Laruelle M, Baldwin RM, Rattner Z, al-Tikriti MS, Zea-Ponce Y, Zoghbi SS, Charney DS, Price JC, Frost JJ, Hoffer PB, et al. (1994). SPECT quantification of [123I]iomazenil binding to benzodiazepine receptors in nonhuman primates: I. Kinetic modeling of single bolus experiments. J Cereb Blood Flow Metab.
17 Laruelle M, Abi-Dargham A, al-Tikriti MS, Baldwin RM, Zea-Ponce Y, Zoghbi SS, Charney DS, Hoffer PB, Innis RB. (1994). SPECT quantification of [123I]iomazenil binding to benzodiazepine receptors in nonhuman primates: II. Equilibrium analysis of constant infusion experiments and correlation with in vitro parameters. J Cereb Blood Flow Metab.
18 Sybirska E, Seibyl JP, Bremner JD, Baldwin RM, al-Tikriti MS, Bradberry C, Malison RT, Zea-Ponce Y, Zoghbi S, During M, et al. (1993). [123I]iomazenil SPECT imaging demonstrates significant benzodiazepine receptor reserve in human and nonhuman primate brain. Neuropharmacology.
19 Zoghbi SS, Baldwin RM, Seibyl JP, al-Tikriti MS, Zea-Ponce Y, Laruelle M, Sybirska EH, Woods SW, Goddard AW, Malison RT, et al. (1992). Pharmacokinetics of the SPECT benzodiazepine receptor radioligand [123I]iomazenil in human and non-human primates. Int J Rad Appl Instrum B.
20 Moriwaki H, Matsumoto M, Hashikawa K, Oku N, Ishida M, Seike Y, Fukuchi K, Hori M, Nishimura T. (1998). Iodine-123-iomazenil and iodine-123-iodoamphetamine SPECT in major cerebral artery occlusive disease. J Nucl Med.
21 Dong Y, Fukuyama H, Nabatame H, Yamauchi H, Shibasaki H, Yonekura Y. (1997). Assessment of benzodiazepine receptors using iodine-123-labeled iomazenil single-photon emission computed tomography in patients with ischemic cerebrovascular disease. A comparison with PET study. Stroke.
22 Dey HM, Seibyl JP, Stubbs JB, Zoghbi SS, Baldwin RM, Smith EO, Zubal IG, Zea-Ponce Y, Olson C, Charney DS, et al. (1994). Human biodistribution and dosimetry of the SPECT benzodiazepine receptor radioligand iodine-123-iomazenil. J Nucl Med.
23 Verhoeff NP, Busemann Sokole E, Hengst D, Stubbs JB, van Royen EA. (1993). Dosimetry of iodine-123 iomazenil in humans. Eur J Nucl Med.
24 Ito H, Goto R, Koyama M, Kawashima R, Ono S, Sato K, Fukuda H. (1996). A simple method for the quantification of benzodiazepine receptors using iodine-123 iomazenil and single-photon emission tomography. Eur J Nucl Med.